# ^99m^Tc-Ethylenediaminediacetic acid/hydrazinonicotinic acid-[DGlu^1^, desGlu^2–6^]minigastrin

Chemical name: | ^99m^Tc-Ethylenediaminediacetic acid/hydrazinonicotinic acid-[DGlu^1^, desGlu^2–6^]minigastrin
Abbreviated name: | ^99m^Tc-EDDA/HYNIC-MG11
Synonym: | ^99m^Tc-Minigastrin, ^99m^Tc-[DGlu^1^, desGlu^2-6^]minigastrin, ^99m^Tc-MG11
Agent Category: | Peptide
Target: | Gastrin/cholecystokinin-2 (CCK-2, CCK-B) receptor
Target Category: | Receptor binding
Method of detection: | Single-photon emission computed tomography (SPECT), planar gamma imaging
Source of signal: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents | ^99m^Tc-EDDA/HYNIC-MG11, a proposed structure not yet confirmed by experiments.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=99mTc-minigastrin%20OR%20%28HYNIC-MG11%29)]

^99m^Tc-Ethylenediaminediacetic acid/hydrazinonicotinic acid-[DGlu^1^, desGlu^2–6^]minigastrin (^99m^Tc-EDDA/HYNIC-MG11) is a radiolabeled peptide developed for single-photon emission computed tomography (SPECT) imaging of tumors that express the gastrin/cholecystokinin-2 (CCK-2) receptor (1). ^99m^Tc is a gamma emitter with a physical half-life (t_½_) of 6.01 h.

The gastrointestinal peptides gastrin and CCK have various regulatory functions in the brain and gastrointestinal tract (2). Gastrin and CCK have the same COOH-terminal pentapeptide amide sequence, which is the biologically active site (3). Human gastrin is a peptide composed of 34 amino acids and also exists in several C-terminal truncated forms (4). These C-terminal truncated forms include minigastrin, which is a 13-residue peptide with the sequence of LEEEEEAYGWMDF-NH_2_. CCKs exist in a variety of biologically active molecular forms that are derived from a precursor molecule comprising 115 amino acids (5). These forms range from 4 to 58 amino acids in length and include sulphated and unsulphated CCK-8, which has the structure DYMGWMDF-NH_2_. They bind to and act through transmembrane G-protein–coupled receptors (6). Two different CCK receptor subtypes have been identified in normal tissues. CCK-1 (CCK-A, alimentary) receptors have low affinity for gastrin, and CCK-2 (CCK-B, brain) receptors have high affinity for gastrin (5). They also differ in terms of molecular structure, distribution, and affinity for CCK. These receptors have also been found to be expressed or overexpressed on a multitude of tumor types (6). CCK-2 receptors have been found most frequently in medullary thyroid carcinoma, small-cell lung cancers, astrocytomas, and stromal ovarian cancers (2). CCK-1 receptors have been identified in gastroenteropancreatic tumors, meningiomas, and neuroblastoma.

Reubi et al. (7) designed a series of radiolabeled CCK-8 peptides that showed high specificity for potential in vivo imaging of tumors expressing CCK-2 receptors. Because of its favorable physical properties, ^99m^Tc is still the radionuclide of choice for routine clinical applications (8). Hydrazinonicotinic acid (HYNIC) is a bifunctional coupling agent for ^99m^Tc labeling of peptides that can achieve high specific activities without interfering with the amino acid sequence responsible for receptor binding (9-11). In this approach, ^99m^Tc is bound to the hydrazine group, and other coordination sites are occupied by one or more coligands. The choice of coligand can influence the stability and hydrophilicity of the radiolabeled peptide. Using the HYNIC labeling strategy and ethylenediaminediacetic acid (EDDA) or tris(hydroxymethyl)-methylglycine (tricine) as the coligand, von Guggenberg et al. (12) reported the success of radiolabeling the MG0 peptide (D-Glu-Glu_5_-Ala-Tyr-Gly-Trp-Met-Asp-PheNH_2_). The ^99m^Tc-EDDA/HYNIC-MG0 peptide showed high tumor uptake in nude mice bearing AR42J tumors, but it also has very high kidney activity. To minimize kidney uptake, the same research group designed a shortened peptide analog by depletion of the five glutamic acid molecules in positions 2–6 to produce ^99m^Tc-EDDA/HYNIC-[DGlu^1^, desGlu^2–6^]minigastrin (^99m^Tc-EDDA/HYNIC-MG11) (1).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=99mTc-minigastrin%20OR%20%28HYNIC-MG11%29)]

von Guggenberg et al. (1) reported the radiosynthesis of ^99m^Tc-EDDA/HYNIC-MG11 by both the EDDA direct labeling and tricine/EDDA exchange labeling methods. Tricine, EDDA, and HYNIC-MG were obtained commercially. The purity of HYNIC-MG was >95%. In the direct radiolabeling procedure, HYNIC-MG (10 μg) was mixed and incubated with EDDA, 400 MBq (10.8 mCi) ^99m^Tc pertechnetate (^99m^TcO_4_−), and stannous chloride in a total volume of 1 ml at pH 6 and 80ºC for 30 min. High-performance liquid chromatography (HPLC) analysis showed a radiochemical purity of >90%. The specific activity was >70 GBq/μmol (>1.89 Ci/μmol). In the tricine/EDDA exchange labeling method, HYNIC-MG was incubated with EDDA/tricine solution (20 mg/ml tricine, 10 mg/ml EDDA), ^99m^TcO_4_−, and stannous chloride (1 mg/ml) in a total volume of 2 ml at pH 6 and 100ºC for 10 min. The labeling yield was <90% and the radiochemical purity was <90%. HPLC analysis showed that only incomplete conversion of the ^99m^Tc-tricine complex into the ^99m^Tc-EDDA complex was achieved. Further purification was achieved by solid-phase extraction with the use of a C18-Sep-Pak-Light cartridge. The authors suggested that the ^99m^Tc-EDDA-HYNIC-MG11 was composed of two EDDA coligand molecules per peptide molecule. They also suggested that impurities exposed by HPLC analysis were products of isomerism and oxidative side products.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=99mTc-minigastrin%20OR%20%28HYNIC-MG11%29)]

The in vitro stability of ^99m^Tc-EDDA/HYNIC-MG11 purified by solid-phase extraction was tested by incubating the radiolabeled peptide (200–1,000 pmol/ml) in phosphate-buffered saline (PBS, pH 7.4), PBS that contained 10,000-fold molar excess of cysteine (cysteine PBS), or fresh human plasma at 37ºC for up to 24 h (1). At 4 h, HPLC analysis showed that the amounts of intact ^99m^Tc-EDDA/HYNIC-MG11 were 98.6%, 91.2%, and 98.1% in the PBS, cysteine PBS, and plasma, respectively. At 24 h, the amounts of intact radiolabeled peptide were 95%, 85.8%, and 89.4% in the PBS, cysteine PBS, and plasma, respectively. Invitro metabolic stability studies of ^99m^Tc-EDDA/HYNIC-MG11 were conducted in rat kidney and liver homogenates (1). The studies showed a very rapid degradation of ^99m^Tc-EDDA/HYNIC-MG11. After 30 min of incubation in the liver homogenates, <5% intact peptide remained. Incubation in the kidney homogenates showed that the degradation was more rapid with <5% intact peptide remaining at 10 min.

The binding affinities of unlabeled EDDA/HYNIC-MG11 and ^99m^Tc-EDDA/HYNIC-MG11 were tested in competition assays against ^125^I-Tyr^12^gastrin by using rat pancreatic tumor AR42J cell membranes as the source of gastrin receptors (1). The inhibition constant (IC_50_) of the unlabeled HYNIC-MG11 was <2 nM, and the dissociation constant (K_d_) of ^99m^Tc-EDDA/HYNIC-MG11 was determined to be 3.97 nM. AR42J cell internalization studies (n = 3) showed that 12 ± 0.21% of the total radioactivity was internalized after 120 min of incubation (1). The radioligand was rapidly internalized after binding with >80%, and 94.4 ± 1.22% internalized fractions of the bound activity were achieved after 15 min and 120 min of incubation, respectively. Externalization experiments (efflux studies; n = 3) showed a very small amount of released radioactivity: 4.02 ± 0.21% after 1.5 h of incubation.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=99mTc-minigastrin%20OR%20%28HYNIC-MG11%29)]

von Guggenberg et al. (1) conducted biodistribution studies of ^99m^Tc-EDDA/HYNIC-MG11 in nude mice bearing AR42J tumors. Each mouse received 1 MBq (27 μCi) ^99m^Tc-EDDA/HYNIC-MG11 (~0.05 μg) radioactivity. In general, the radiolabeled peptide was mainly excreted by the kidneys and was rapidly eliminated from most organs. The radioactivity levels for the tumor were 4.77 ± 0.72% injected dose/g (% ID/g) and 7.11 ± 0.22% ID/g at 1 h and 4 h, respectively. These levels decreased to 1.37 ± 0.54% ID/g and 1.10 ± 0.26% ID/g when 50 μg human minigastrin I (MGh) was coinjected with the radioligand. The kidney activities were 2.44 ± 0.97% ID/g and 1.96 ± 0.14% ID/g at 1 h and 4 h, respectively. These levels slightly decreased to 2.18 ± 0.40% ID/g and 1.54 ± 0.16% ID/g with the blocking of MGh. This was a 98% reduction in the kidney radioactivity level when compared with that of the ^99m^Tc-EDDA/HYNIC-MG0 peptide. The other major organ radioactivity levels (% ID/g) at 4 h were 1.26 ± 0.07 (liver), 0.90 ± 0.23 (intestine), 0.46 ± 0.23 (stomach), 0.49 ± 0.10 (spleen), 0.15 ± 0.05 (lung), 0.11 ± 0.14 (blood), 0.09 ± 0.04 (pancreas), and 0.02 ± 0.02 (muscle). A significant reduction in radioactivity levels as a result of MGh coinjection was observed in receptor-expressing organs (stomach and pancreas).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2899mTc-minigastrin%20OR%20%28HYNIC-MG11%29%29%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2899mTc-minigastrin%20OR%20%28HYNIC-MG11%29%29%20AND%20%28primate%20NOT%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2899mTc-minigastrin%20OR%20%28HYNIC-MG11%29%29%20AND%20human)]

No publication is currently available.

## References

1. von Guggenberg, E., H. Dietrich, I. Skvortsova, M. Gabriel, I.J. Virgolini, and C. Decristoforo, (99m)Tc-labelled HYNIC-minigastrin with reduced kidney uptake for targeting of CCK-2 receptor-positive tumours. Eur J Nucl Med Mol Imaging, 2007.
2 Reubi J.C., Schaer J.C., Waser B. (1997). Cholecystokinin(CCK)-A and CCK-B/gastrin receptors in human tumors. Cancer Res.
3 Aly A., Shulkes A., Baldwin G.S. (2004). Gastrins, cholecystokinins and gastrointestinal cancer. Biochim Biophys Acta.
4 Mather S.J., McKenzie A.J., Sosabowski J.K., Morris T.M., Ellison D., Watson S.A. (2007). Selection of radiolabeled gastrin analogs for Peptide receptor-targeted radionuclide therapy. J Nucl Med.
5 Wang H., Wong P.T., Spiess J., Zhu Y.Z. (2005). Cholecystokinin-2 (CCK2) receptor-mediated anxiety-like behaviors in rats. Neurosci Biobehav Rev.
6 Behr T.M., Behe M.P. (2002). Cholecystokinin-B/Gastrin receptor-targeting peptides for staging and therapy of medullary thyroid cancer and other cholecystokinin-B receptor-expressing malignancies. Semin Nucl Med.
7 Reubi J.C., Waser B. (1996). Unexpected high incidence of cholecystokinin-B/gastrin receptors in human medullary thyroid carcinomas. Int J Cancer.
8 Aloj L., Panico M.R., Caraco C., Zannetti A., Del Vecchio S., Di Nuzzo C., Arra C., Morelli G., Tesauro D., De Luca S., Pedone C., Salvatore M. (2002). Radiolabeling approaches for cholecystokinin B receptor imaging. Biopolymers.
9 Liu S., Edwards D.S. (1999). 99mTc-Labeled Small Peptides as Diagnostic Radiopharmaceuticals. Chem Rev.
10 Decristoforo C., Melendez-Alafort L., Sosabowski J.K., Mather S.J. (2000). 99mTc-HYNIC-[Tyr3]-octreotide for imaging somatostatin-receptor-positive tumors: preclinical evaluation and comparison with 111In-octreotide. J Nucl Med.
11 Barrett J.A., Crocker A.C., Damphousse D.J., Heminway S.J., Liu S., Edwards D.S., Lazewatsky J.L., Kagan M., Mazaika T.J., Carroll T.R. (1997). Biological evaluation of thrombus imaging agents utilizing water soluble phosphines and tricine as coligands when used to label a hydrazinonicotinamide-modified cyclic glycoprotein IIb/IIIa receptor antagonist with 99mTc. Bioconjug Chem.
12 von Guggenberg E., Behe M., Behr T.M., Saurer M., Seppi T., Decristoforo C. (2004). 99mTc-labeling and in vitro and in vivo evaluation of HYNIC- and (Nalpha-His)acetic acid-modified [D-Glu1]-minigastrin. Bioconjug Chem.